# Saposin C-dioleylphosphatidylserine nanovesicles coupled with iron oxides

Chemical name: | Saposin C-dioleylphosphatidylserine nanovesicles coupled with iron oxides
Abbreviated name: | SapC-DOPS-IO
Synonym:
Agent Category: | Nanoparticles
Target: | Phospholipids
Target Category: | Lipids
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging)]

The saposin C (SapC)-dioleylphosphatidylserine (DOPS) nanovesicle coupled with iron oxide, abbreviated as SapC-DOPS-IO, is a contrast agent developed by Kaimal et al. for extracellular phospholipid (PS)-targeted magnetic resonance imaging (MRI) (1).

Saposins are a group of water-soluble lysosomal glycoproteins (SapA, SapB, SapC, and SapD) with molecular weights of 8–11 kDa (1-3). They are generated by the proteolytic processing of the common precursor prosaposin. Saposins localize primarily in the lysosomes and are required for the catabolism of glycosphingolipids (4, 5). The four saposins have a high degree of structural similarity and share lipid-binding and membrane-perturbing properties; however, they behave differently and exhibit different specificities (2, 3). SapC is the second saposin to be discovered, and it binds to membranes in a pH-controlled manner (6). SapC can directly activate enzymes and stimulate the hydrolysis of glycocerebroside and galactocerebroside (7). Deficiency of SapC leads to an abnormal juvenile form of Gaucher disease with accumulation of glucosylceramide in various organs, including the brain (5).

SapC preferentially interacts with unsaturated, negatively charged PS such as DOPS at acidic pH (6, 8). PS is present in all cells and constitutes ~2%–10% of total cellular lipids. In normal tissues, PS is localized in the cell membrane leaflets that face the cytosol. However, in pathological conditions such as tumors, PS translocates to the outer leaflet of the plasma membrane, where it activates and participates in various cellular processes, including apoptosis and necrosis (9). Phagocytes in healthy tissues rapidly and efficiently remove the PS-expressing cells and cell remnants, but these PS-expressing cells and cell remnants accumulate in diseased tissues as a result of the activation of the cell death process and the insufficient clearance of cells with externalized PS (9).

Because tumors express abundant PS on the cell surface and have a lower extracellular pH (pH ~6) than normal tissues (pH ~7), the SapC-PS interaction provides a valuable system for targeted tumor imaging and therapy (4, 9, 10). Qi et al. developed a SapC-DOPS nanovesicle system that induced apoptosis of tumor cells in vitro and inhibited growth of neuroblastomas and malignant peripheral nerve sheath tumors in animal models (2). Fluorescently labeled SapC-DOPS (CVM-SapC-DOPS) has been shown to preferentially accumulate in tumor xenografts (1, 2). Kaimal et al. synthesized SapC-DOPS-IO by encapsulating IO particles into the SapC-DOPS nanovesicles, and they showed that SapC-DOPS-IO was effectively detected in tumors with the use of MRI (1). These studies indicate that SapC-DOPS nanovesicles are promising as a new and robust theranostic agent for cancer-selective detection, visualization, and therapy (1, 2). This chapter summarizes the data obtained with SapC-DOPS-IO. The data obtained with CVM-SapC-DOPS (http://www.ncbi.nlm.nih.gov/books/NBK5330/) are summarized in another chapter in MICAD.

### Related Resource Links:

- Protein information for saposin C (http://www.ncbi.nlm.nih.gov/protein/?term=saposin+C)
- Protein information for prosaposin (http://www.ncbi.nlm.nih.gov/protein?term=prosaposin)
- Saposin-related compounds in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=saposin)
- Saposin-related articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=saposin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

Qi et al. described the synthesis of SapC-DOPS nanovesicles in detail (2). Briefly, recombinant human SapC was expressed in Escherichia coli cells. Pure SapC was then mixed with lipids in acid buffer (pH 5). The protein–lipid mixture was gently sonicated and ultracentrifuged to produce SapC-DOPS nanovesicles in pellet form. No SapC was detected in the supernatant fraction, indicating a very high loading/coupling efficiency. The sonicated SapC-DOPS complexes contained monodispersed, unilamellar vesicles with a mean diameter of ~190 nm.

To encapsulate IO particles (ferumoxtran-10; ~20 nm in diameter) in nanovesicles, Kaimal et al. first oxidized the dextran coating on the IO particles to generate aldehyde groups (1). The oxidized IO particles were then mixed with SapC and lipids to generate SapC-DOPS-IO nanovesicles. The surface aldehydes of the IO particles could form covalent Schiff bonds at high pH with amines of DOPS. The vesicles were sized by passing through a 200-nm polycarbonate membrane. To remove the IO particles attached to the outer surface of the vesicles, the solution was dialyzed against a low pH solution (pH 4.5) of sodium chloride and sodium citrate. The unencapsulated IO particles were removed by passing the solution through a Con-A Sepharose 4B column. The SapC-DOPS-IO nanovesicles were stabilized in 4-(2-hydroxyethyl)-1-piperazine ethanesulfonic acid buffered to pH 8 (20 mM final concentration).

The SapC-DOPS-IO nanovesicles were bilayer-spherical in shape and had a mean diameter of ~200 ± 27 nm. The molar ratio of SapC/DOPS and the mean iron concentration in the SapC-DOPS-IO were determined to be 1:10 and 94.8 ± 12.8 μg/ml, respectively. The relaxivity r_2_ value was measured to be 101.21 ± 4.9 mM^-1^s^-1^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

MRI and inductively coupled plasma-atomic emission spectroscopy (ICP-AES) were performed after incubation of human neuroblastoma cells (CHLA-20) with SapC-DOPS-IO nanovesicles for various times (1). MRI scans of the cells fixed in agarose showed an increasing number of signal voids in cells incubated with SapC-DOPS-IO for longer periods. The R2 and R2* relaxation rates of cells in agarose were 14.64 s^-1^ and 26.74 s^-1^, respectively, for cells exposed to SapC-DOPS-IO, and 7.84 s^-1^ and 11.04 s^-1^, respectively, for control cells exposed to free IO particles for 24 h. The average cellular iron content was 1.48, 2.12, and 3 pg/cell for cells incubated with SapC-DOPS-IO for 12, 18, and 24 h, respectively. When the cells were exposed to various concentrations of SapC-DOPS-IO for 12 h, the cell uptake was proportional to the initial concentration in the growth medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=saposin%20and%20imaging%20and%20therapy)]

Kaimal et al. performed MRI with SapC-DOPS-IO in nude mice bearing neuroblastoma xenografts on the right flank (n = 5 mice) (1). Control animals were injected with phosphate-buffered saline (n = 5 mice). T2*-Weighted imaging at 7T showed that the signal intensity in tumors dropped immediately after injection of SapC-DOPS-IO and gradually decreased further before rebounding slightly 24 h later. The drop in signal intensity was observed over the entire tumor. ICP-AES analysis showed that the concentration of iron in the tumor of a mouse injected with SapC-DOPS-IO was approximately five-fold higher than the concentration of iron in the tumor of a control mouse.

The T2 value in the area of tumors was measured in mice with pancreatic tumor xenografts (MiaPaCa-2) (n = 5 mice). The T2 value before injection of SapC-DOPS-IO was 91.4 ± 11.6 ms. An average drop of 29 ms was seen at 4 h after injection (T2 = 62.8 ± 8.6 ms). In contrast, there was little change in the tumor signal intensity before and 4 h after injection in the control mice (n = 5) injected with free IO or with DOPS-IO not containing SapC. The tumor T2 value between experimental and control mice was significantly different (P = 0.011) (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Kaimal, V., Z. Chu, Y.Y. Mahller, B. Papahadjopoulos-Sternberg, T.P. Cripe, S.K. Holland, and X. Qi, Saposin C Coupled Lipid Nanovesicles Enable Cancer-Selective Optical and Magnetic Resonance Imaging. Mol Imaging Biol, 2010
2 Qi X., Chu Z., Mahller Y.Y., Stringer K.F., Witte D.P., Cripe T.P. (2009). Cancer-selective targeting and cytotoxicity by liposomal-coupled lysosomal saposin C protein. Clin Cancer Res.
3 Rossmann M., Schultz-Heienbrok R., Behlke J., Remmel N., Alings C., Sandhoff K., Saenger W., Maier T. (2008). Crystal structures of human saposins C andD: implications for lipid recognition and membrane interactions. Structure.
4 Wang Y., Grabowski G.A., Qi X. (2003). Phospholipid vesicle fusion induced by saposin C. Arch Biochem Biophys.
5 Atrian S., Lopez-Vinas E., Gomez-Puertas P., Chabas A., Vilageliu L., Grinberg D. (2008). An evolutionary and structure-based docking model for glucocerebrosidase-saposin C and glucocerebrosidase-substrate interactions - relevance for Gaucher disease. Proteins.
6 Abu-Baker S., Qi X., Newstadt J., Lorigan G.A. (2005). Structural changes in a binary mixed phospholipid bilayer of DOPG and DOPS upon saposin C interaction at acidic pH utilizing 31P and 2H solid-state NMR spectroscopy. Biochim Biophys Acta.
7 Nieh M.P., Pencer J., Katsaras J., Qi X. (2006). Spontaneously forming ellipsoidal phospholipid unilamellar vesicles and their interactions with helical domains of saposin C. Langmuir.
8 Abu-Baker S., Qi X., Lorigan G.A. (2007). Investigating the interaction of saposin C with POPS and POPC phospholipids: a solid-state NMR spectroscopic study. Biophys J.
9 Schutters K., Reutelingsperger C. (2010). Phosphatidylserine targeting for diagnosis and treatment of human diseases. Apoptosis.
10 Zhang X., Lin Y., Gillies R.J. (2010). Tumor pH and its measurement. J Nucl Med.